# ^123^I-c(RGDfK)-human serum albumin-tissue inhibitor of matrix metalloproteinase 2 fusion protein

Chemical name: | ^123^I-c(RGDfK)-human serum albumin-tissue inhibitor of matrix metalloproteinase 2 fusion
Abbreviated name: | ^123^I-RGD-HSA-TIMP2
Synonym: | ^123^I-RGDfK-HSA-TIMP2
Agent category: | Protein
Target: | α_v_β_3_ integrin receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/contrast: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD-HSA-TIMP-2)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (4-7). MMP expression is highly regulated in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (8). There are four members of endogenous tissue inhibitors of metalloproteinases (TIMPs), which regulate the activity of MMPs leading to inhibition of tumor growth and metastasis (9, 10). TIMP-2 (TIMP2) is a bifunctional inhibitor of angiogenesis by inhibition of proteinase activity of MMPs and endothelial cell proliferation via binding to α_3_β_1_ (the N-terminal domain) and by MMP-independent anti-angiogenic activity (the C-terminal domain) (11, 12). Kang et al. (13) fused the N-terminal domain of TIMP2 to the C-terminus of human serum albumin (HSA) to form HSA/TIMP2 fusion protein (HSA-TIMP2), which is readily secreted by the transfected yeast Saccharomyces cerevisiae. HSA-TIMP2 retains its anti-angiogenic activity at the C-terminal domain with little MMP inhibitory activity at the N-terminal domain. Lee et al. (14) have evaluated Cy5.5-HSA/TIMP2 (Cy5.5-HSA-TIMP2) for in vivo near-infrared (NIR) fluorescence imaging of rat prostate MLL tumors in nude mice showing maximum tumor accumulation at 2 d after injection.

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (15). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (16-21). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents (18, 22, 23). Various radiolabeled RGD peptides (antagonists) have been introduced for imaging of tumors and tumor angiogenesis (24). Choi et al. (25) conjugated multiple c(RGDfK) peptides to HSA-TIMP2 to enhance the binding capacity of the protein (RGD-HSA-TIMP2) to tumors and their vasculatures. ^123^I-RGD-HSA-TIMP2 and ^123^I-HSA-TIMP2 have been studied as potential single-photon emission computed tomography (SPECT) probes for imaging α_v_β_3_ receptors in nude mice bearing human glioblastoma U87MG tumors.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D), TIMP (http://www.ncbi.nlm.nih.gov/books?term=TIMP%20AND%20micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (TIMP2 (http://www.ncbi.nlm.nih.gov/gene/7077), HSA (http://www.ncbi.nlm.nih.gov/gene/213), α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), α_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3675), β_1_ integrin (http://www.ncbi.nlm.nih.gov/gene/3688), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (TIMP2 (http://omim.org/entry/188825), HSA (http://omim.org/entry/103600), α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), α_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/605025), β_1_ integrin (http://www.ncbi.nlm.nih.gov/omim/135630), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (TIMP (http://www.clinicaltrials.gov/ct2/results?term=TIMP), RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (TIMP (http://google2.fda.gov/search?q=TIMP&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*), RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2)]

HSA-TIMP2 (0.23 µmol) and c[RGDfK(COCH_2_SH)] (1.39 µmol) were incubated with N-succinimidyl iodoacetate (3.52 µmol) to form a thioether linkage between the RGD peptide and HSA-TIMP2 protein (25). RGD-HSA-TIMP2 was purified with column chromatography. The molecular weights of RGD-HSA-TIMP2 and HSA-TIMP2 were calculated to be 88.42 kDa and 92.78 kDa with mass spectroscopy, respectively. There were 6 RGD molecules per RGD-HSA-TIMP2. ^123^I-RGD-HSA-TIMP2 and ^123^I-HSA-TIMP2 were prepared with the Iodogen method by incubation of ~11 nmol protein with 185 MBq (5 mCi) [^123^I]NaI for 20 min at room temperature. The radiochemical yields were 45%–50%. The specific activities of ^123^I-RGD-HSA-TIMP2 and ^123^I-HSA-TIMP2 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20in%20vitro)]

Flow cytometry analysis showed that 45% and 91% of U89MG cells were positive after incubation with HSA-TIMP2-FITC and RGD-HSA-TIMP2-FITC for 24 h at 4°C (25), respectively. Confocal microscopy showed internalization of fluorescence activity inside the cells incubated with 1.6 nM RGD-HSA-TIMP2-FITC for 3 h at 37°C but not with HSA-TIMP2-FITC. No blocking studies were performed with unlabeled RGD-HSA-TIMP2.

In vitro cell viability of U87MG was assessed after incubation with various concentrations (0.11–3.2 nM) of RGD, HSA-TIMP2, and RGD-HSA-TIMP2 for 24 h at 37°C (25). The cell viability values with 3.2 nM RGD, HSA-TIMP2, and RGD-HSA-TIMP2 were 92.5 ± 4.0%, 73.5 ± 7.9% (P < 0.05 versus RGD), and 66.7 ± 0.6% (P < 0.001 versus RGD), respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20rodentia)]

Choi et al. (25) performed whole-body SPECT/CT imaging in nude mice (the number of mice was not reported) bearing U87MG tumors at 1 h and 4 h after intravenous injection of 18.5 MBq (0.5 mCi) ^123^I-RGD-HSA-TIMP2 or ^123^I-HSA-TIMP2. Little tumor accumulation of ^123^I-HSA-TIMP2 was observed at 1 h and 4 h. The tumor accumulation of ^123^I-RGD-HSA-TIMP2 was slightly higher than that of ^123^I-HSA-TIMP2, with poor tumor contrast. High liver accumulation for both tracers was observed. Immunofluorescence staining of tumor tissue sections showed an increase in CD31 (endothelial cell biomarker) expression in the tumor tissue.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
9 Baker A.H., Edwards D.R., Murphy G. (2002). Metalloproteinase inhibitors: biological actions and therapeutic opportunities. J Cell Sci.
10 Jiang Y., Goldberg I.D., Shi Y.E. (2002). Complex roles of tissue inhibitors of metalloproteinases in cancer. Oncogene.
11 Fernandez C.A., Butterfield C., Jackson G., Moses M.A. (2003). Structural and functional uncoupling of the enzymatic and angiogenic inhibitory activities of tissue inhibitor of metalloproteinase-2 (TIMP-2): loop 6 is a novel angiogenesis inhibitor. J Biol Chem.
12 Seo D.W., Li H., Guedez L., Wingfield P.T., Diaz T., Salloum R., Wei B.Y., Stetler-Stevenson W.G. (2003). TIMP-2 mediated inhibition of angiogenesis: an MMP-independent mechanism. Cell.
13 Kang W.K., Park E.K., Lee H.S., Park B.Y., Chang J.Y., Kim M.Y., Kang H.A., Kim J.Y. (2007). A biologically active angiogenesis inhibitor, human serum albumin-TIMP-2 fusion protein, secreted from Saccharomyces cerevisiae. Protein Expr Purif.
14 Lee M.S., Kim Y.H., Kim Y.J., Kwon S.H., Bang J.K., Lee S.M., Song Y.S., Hahm D.H., Shim I., Han D., Her S. (2011). Pharmacokinetics and biodistribution of human serum albumin-TIMP-2 fusion protein using near-infrared optical imaging. J Pharm Pharm Sci.
15 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
16 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
17 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
18 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
19 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
20 Varner J.A., Cheresh D.A. (1996). Integrins and cancer. Curr Opin Cell Biol.
21 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
22 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
23 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
24 Haubner R., Beer A.J., Wang H., Chen X. (2010). Positron emission tomography tracers for imaging angiogenesis. Eur J Nucl Med Mol Imaging.
25 Choi N., Kim S.M., Hong K.S., Cho G., Cho J.H., Lee C., Ryu E.K. (2011). The use of the fusion protein RGD-HSA-TIMP2 as a tumor targeting imaging probe for SPECT and PET. Biomaterials.